# 2-(4-(2-[^18^F]Fluoroethyl)piperidin-1-yl)benzo[4,5]imidazo[1,2-a]pyrimidine

Chemical name: | 2-(4-(2-[^18^F]Fluoroethyl)piperidin-1-yl)benzo[4,5]imidazo[1,2-a]pyrimidine
Abbreviated name: | [^18^F]T808
Synonym:
Agent category: | Compound
Target: | Tau plaques
Target category: | Acceptor
Method of detection: | Positron emission tomography (PET)
Source of signal: | ^18^F
Activation: | No
Studies: | - In vitro; - Rodents | Click on the above structure for additional information in PubChem (http://pubchem.ncbi.nlm.nih.gov/).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=T808)]

Alzheimer's disease (AD) is a form of dementia with a gradual memory loss and a progressive decline in mental functions over time (1, 2). It is characterized pathologically by neuronal loss, extracellular senile plaques (aggregates of amyloid-β (Aβ) peptides consisting of 40–42 amino acids formed as the proteolytic cleavage of Aβ protein precursor (AβPP)), and intracellular neurofibrillary tangles (filaments of microtubule-binding hyper-phosphorylated protein tau) in the brain, especially in the hippocampus and associative regions of the cortex (3, 4). Aβ plaques and tau neurofibrillary tangles are implicated as the main causes of neuronal degeneration and cell death in AD patients (5, 6).

Early diagnosis of AD is important for treatment consideration and disease management (7). Various Aβ imaging agents have been developed for magnetic resonance imaging, single-photon emission computed tomography, and positron emission tomography (PET) (8-14). The binding properties of different derivatives of Congo red, thioflavin, stibene, and aminonaphthalene have been studied in postmortem human brain tissue and in transgenic mice (Nesterov, E.E., 2005; Ran, C., 2009). Of these analogs, 2-(1-(6-[(2-[^18^F]fluoroethyl)(methyl)amino]-2-naphthyl)ethylidene)malono nitrile ([^18^F]FDDNP) has been studied in humans, showing more binding in the brains of patients with AD than in those of healthy people (15). [^18^F]FDDNP has been found to bind to both Aβ plaques and tau neurofibrillary tangles. However, [^18^F]FDDNP exhibits low signal/noise ratios for PET imaging because it is highly lipophilic. N-methyl-[^11^C]-2-(4'-methylaminophenyl)-6-hydroxybenzothiasole, an Aβ-binding compound based on a series of neutral thioflavin-T derivatives, was radiolabeled with the positron-emitting radionuclide ^11^C ([^11^C]6-OH-BTA-1 or [^11^C]PIB). [^11^C]6-OH-BTA-1 was found to be a promising imaging agent for Aβ plaques in the brain (10). Okamura et al. (16) identified a series of quinolone derivatives that bind tau neurofibrillary tangles with higher affinity than Aβ plaques. One of these derivatives, 2-(4-aminophenyl)-6-(2-([^18^F]fluoroethoxy))quinolone ([^18^F]THK523), was shown with PET imaging to have higher brain accumulation in tau transgenic mice than in Aβ transgenic mice (17). Zhang et al. (18) evaluated 2-(4-(2-[^18^F]fluoroethyl)piperidin-1-yl)benzo[4,5]imidazo[1,2-a]pyrimidine ([^18^F]T808) as a PET imaging agent for tau pathologies.

### Related Resource Links:

- Chapters in MICAD (amyloid (http://www.ncbi.nlm.nih.gov/sites/entrez?db=Books&cmd=Search&term=amyloid+AND+micad%5bbook%5d&doptcmdl=TOCView&log%24=booksrch&bname=micad), tau (http://www.ncbi.nlm.nih.gov/sites/entrez?db=Books&cmd=Search&term=tau+AND+micad%5bbook%5d&doptcmdl=TOCView&log%24=booksrch&bname=micad))
- Gene information in NCBI (amyloid (http://www.ncbi.nlm.nih.gov/gene/351), tau (http://www.ncbi.nlm.nih.gov/gene/4137))
- Articles in Online Mendelian Inheritance in Man (OMIM) (amyloid (http://www.ncbi.nlm.nih.gov/omim/104760), tau (http://www.ncbi.nlm.nih.gov/omim/157140))
- Clinical trials (amyloid (http://www.clinicaltrials.gov/ct2/results?term=Amyloid), tau (http://www.clinicaltrials.gov/ct2/results?term=tau+imaging))
- Drug information in FDA (amyloid inhibitors (http://google2.fda.gov/search?q=Amyloid+inhibitor&client=FDAgov&site=FDAgov&lr=&proxystylesheet=FDAgov&output=xml_no_dtd&getfields=*&x=16&y=16), tau inhibitors (http://google2.fda.gov/search?q=tau+inhibitor&client=FDAgov&site=FDAgov&lr=&proxystylesheet=FDAgov&output=xml_no_dtd&getfields=*&x=11&y=7))

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=T808%20and%20synthesis)]

[^18^F]T808 was readily synthesized with standard ^18^F-fluorination of the tosylate precursor ([^18^F]KF/Kryptofix2.2.2; 5 min at 90°C) (18). [^18^F]T808 was purified with high-performance liquid chromatography. Average yield (n = 24) was 37.4%, with an average specific activity of 255 GBq/µmol (6.9 Ci/µmol) at the end of synthesis and a radiochemical purity of >98%. Total synthesis time was ~90 min. The Log P (lipophilicity) value of [^18^F]T808 was not reported.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=T808%20and%20in%20vitro)]

Zhang et al. (18) performed radioautographic binding studies of [^18^F]T808 in postmortem brain (frontotemporal cortex) tissues of AD patients (n = 33, age 64–93 years) and normal control patients (n = 12, age 64–89 years). [^18^F]T808 localized in the "tau-rich" sections, whereas there was minimal staining in the "tau-poor/Aβ-rich" sections. The "tau-rich"/"tau-poor/Aβ-rich" ratio was determined to be 27. [^18^F]T808 radioactivity levels colocalized with immunostaining for tau in the frontal and cingulate areas, with little colocalization with Aβ_42_. Saturation binding autoradiography exhibited a K_d_ value of 22 nM, whereas a K_d_ value for Aβ could not be determined due to weak binding of [^18^F]T808 to Aβ plaques.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=T808%20and%20rodentia)]

Zhang et al. (18) performed PET imaging over 30 minutes after intravenous injection of 7.4 MBq (200 μCi) [^18^F]T808 into wild-type mice (n = 11) or 14.8 MBq (400 μCi) [^18^F]T808 into wild-type rats (n = 11). [^18^F]T808 showed an initial rapid penetration into the mouse brain, with 6.7% injected dose (ID)/g at 2.5 min and a quick washout (2.3% ID/g at 20 min). Similar kinetics was observed in the rats, with 0.7% ID/g and 0.1% ID/g at 2.5 min and 20 min after injection. Some bone accumulation was observed in the mice.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=T808%20and%20%28dog%20or%20pig%20or%20cat%20or%20rabbit%20or%20sheep%29)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=T808%20and%20primate%20not%20human)]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=T808%20and%20humans)]

No publication is currently available.

## References

1 Forstl H., Kurz A. (1999). Clinical features of Alzheimer's disease. Eur Arch Psychiatry Clin Neurosci.
2 Heininger K. (2000). A unifying hypothesis of Alzheimer's disease. IV. Causation and sequence of events. Rev Neurosci.
3 Hardy J.A., Higgins G.A. (1992). Alzheimer's disease: the amyloid cascade hypothesis. Science.
4 Mirra S.S., Heyman A., McKeel D., Sumi S.M., Crain B.J., Brownlee L.M., Vogel F.S., Hughes J.P., van Belle G., Berg L. (1991). The Consortium to Establish a Registry for Alzheimer's Disease (CERAD). Part II. Standardization of the neuropathologic assessment of Alzheimer's disease. Neurology.
5 Brandt R., Hundelt M., Shahani N. (2005). Tau alteration and neuronal degeneration in tauopathies: mechanisms and models. Biochim Biophys Acta.
6 Hardy J. (2003). The relationship between amyloid and tau. J Mol Neurosci.
7 de Leon M.J., DeSanti S., Zinkowski R., Mehta P.D., Pratico D., Segal S., Clark C., Kerkman D., DeBernardis J., Li J., Lair L., Reisberg B., Tsui W., Rusinek H. (2004). MRI and CSF studies in the early diagnosis of Alzheimer's disease. J Intern Med.
8 Bacskai B.J., Klunk W.E., Mathis C.A., Hyman B.T. (2002). Imaging amyloid-beta deposits in vivo. J Cereb Blood Flow Metab.
9 Mathis C.A., Wang Y., Holt D.P., Huang G.F., Debnath M.L., Klunk W.E. (2003). Synthesis and evaluation of 11C-labeled 6-substituted 2-arylbenzothiazoles as amyloid imaging agents. J Med Chem.
10 Mathis C.A., Wang Y., Klunk W.E. (2004). Imaging beta-amyloid plaques and neurofibrillary tangles in the aging human brain. Curr Pharm Des.
11 Kung M.P., Hou C., Zhuang Z.P., Skovronsky D., Kung H.F. (2004). Binding of two potential imaging agents targeting amyloid plaques in postmortem brain tissues of patients with Alzheimer's disease. Brain Res.
12 Nordberg A. (2004). PET imaging of amyloid in Alzheimer's disease. Lancet Neurol.
13 Wang Y., Klunk W.E., Debnath M.L., Huang G.F., Holt D.P., Shao L., Mathis C.A. (2004). Development of a PET/SPECT agent for amyloid imaging in Alzheimer's disease. J Mol Neurosci.
14 Bacskai B.J., Hickey G.A., Skoch J., Kajdasz S.T., Wang Y., Huang G.F., Mathis C.A., Klunk W.E., Hyman B.T. (2003). Four-dimensional multiphoton imaging of brain entry, amyloid binding, and clearance of an amyloid-beta ligand in transgenic mice. Proc Natl Acad Sci U S A.
15 Shoghi-Jadid K., Small G.W., Agdeppa E.D., Kepe V., Ercoli L.M., Siddarth P., Read S., Satyamurthy N., Petric A., Huang S.C., Barrio J.R. (2002). Localization of neurofibrillary tangles and beta-amyloid plaques in the brains of living patients with Alzheimer disease. Am J Geriatr Psychiatry.
16 Okamura N., Suemoto T., Furumoto S., Suzuki M., Shimadzu H., Akatsu H., Yamamoto T., Fujiwara H., Nemoto M., Maruyama M., Arai H., Yanai K., Sawada T., Kudo Y. (2005). Quinoline and benzimidazole derivatives: candidate probes for in vivo imaging of tau pathology in Alzheimer's disease. J Neurosci.
17 Fodero-Tavoletti M.T., Okamura N., Furumoto S., Mulligan R.S., Connor A.R., McLean C.A., Cao D., Rigopoulos A., Cartwright G.A., O'Keefe G., Gong S., Adlard P.A., Barnham K.J., Rowe C.C., Masters C.L., Kudo Y., Cappai R., Yanai K., Villemagne V.L. (2011). 18F-THK523: a novel in vivo tau imaging ligand for Alzheimer's disease. Brain.
18 Zhang W., Arteaga J., Cashion D.K., Chen G., Gangadharmath U., Gomez L.F., Kasi D., Lam C., Liang Q., Liu C., Mocharla V.P., Mu F., Sinha A., Szardenings A.K., Wang E., Walsh J.C., Xia C., Yu C., Zhao T., Kolb H.C. (2012). A Highly Selective and Specific PET Tracer for Imaging of Tau Pathologies. J Alzheimers Dis.